# ^64^Cu-4,11-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-p-Cl-Phe-cyclo(D-Cys-Tyr-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)D-Tyr-NH_2_

Chemical name: | ^64^Cu-4,11-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-p-Cl-Phe-cyclo(D-Cys-Tyr-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)D-Tyr-NH_2_
Abbreviated name: | ^64^Cu-CB-TE2A-LM3
Synonym:
Agent category: | Peptide
Target: | Somatostatin receptor 2 (SSTR2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=47117741), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=71979669) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6750) for more information about somatostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CB-TE2A-LM3)]

Somatostatin (SST) is an inhibitor of the release of somatotropin, glucagon, insulin, gastrointestinal hormones, and other secretory proteins (1). SST is also known as somatotropin release-inhibiting factor (SRIF). SSTR is a cyclic polypeptide with two biologically active isoforms, SRIF-14 and SRIF-28, of 14 and 28 amino acids, respectively. SRIF has a short plasma half-life of <3 min (2). SSTR receptors (SSTRs) (G-protein–coupled) have been found on a variety of neuroendocrine tumors and cells of the immune system, and five individual subtypes (SSTR1–SSTR5) have been identified and subsequently cloned from animal and human tissues (3, 4). SSTR also inhibits cell proliferation and promotes apoptosis through binding to specific cell-surface SSTRs (5).

^111^In-Diethylenetriamine pentaacetic acid-octreotide (^111^In-DTPA-OCT) is an SST analog that, over the last decade, has remained the most widely used radiopharmaceutical and the only FDA approved radiotracer for the scintigraphic detection and staging of primary and metastatic neuroendocrine tumors bearing SSTRs with single-photon emission computed tomography (SPECT) (6). It has also shown promising results in peptide-receptor radionuclide therapy (7). Octreotide (OCT) is a cyclic peptide with eight amino acids. ^111^In-DTPA-OCT binds with high affinity to SSTR2 and SSTR5 and to SSTR3 to a lesser degree, but it does not bind to SSTR1 and SSTR4 (8). A large number of radiolabeled SST analogs have been reported using different radionuclides and different linkers. Currently used targeting SSTR peptides mainly are SSTR2 agonists. Therefore, there is a need for SSTR2 antagonist radioligands (9). p-Cl-Phe-cyclo(D-Cys-Tyr-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)D-Tyr-NH_2_ (LM3) is a novel selective SSTR2 antagonist. Fani et al. (10) prepared ^64^Cu-4,11-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-LM3 (^64^Cu-CB-TE2A-LM3) as a positron emission tomography (PET) imaging agent for SSTR2.

### Related Resource Links:

- Chapters in MICAD (Somatostatin (http://www.ncbi.nlm.nih.gov/books?term=Somatostatin%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Somatostatin (http://www.ncbi.nlm.nih.gov/gene/6750), SSTR2 (http://www.ncbi.nlm.nih.gov/gene/6752))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Somatostain (http://omim.org/entry/182450), SSTR2 (http://omim.org/entry/182452))
- Clinical trials (Somatostatin receptor (http://www.clinicaltrials.gov/ct2/results?term=somatostatin+receptor))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CB-TE2A-LM3+and+synthesis)]

CB-TE2A-LM3 was synthesized via standard solid-phase peptide synthesis with a calculated mass of 1,490.9 Da in agreement with mass spectrometry (10). CB-TE2A was incorporated at the N-terminus of the peptide. CB-TE2A-LM3 was purified with high-performance liquid chromatography. ^64^Cu was complexed to CB-TE2A-LM3 by reaction of CB-TE2A-LM3 with ^64^CuCl_2_ in ammonium acetate (pH 8.0) for 30 min at 95°C. ^64^Cu-CB-TE2A-LM3 had a >95% radiochemical purity and a specific activity of 15 MBq/nmol (0.41 mCi/nmol) with labeling yield >95%. ^64^Cu-CB-TE2A-LM3 had a log D value of -1.36 ± 0.25 and a net charge of +2.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CB-TE2A-LM3+and+in+vitro)]

Fani et al. (10) reported that ^nat^Cu-CB-TE2A-LM3 had 50% inhibition concentration (IC_50_) values of >1,000, 4.2 ± 1.6, >1,000, >1,000, and >1,000 nM for human SSTR1, SSTR2, SSTR3, SSTR4, and SSTR5 receptors in competition with ^125^I-SRIF-28, respectively. Immunofluorescence studies showed that [Tyr^3^]octreotide (10 nM) triggers receptor internalization whereas ^nat^Ga-NODAGA-LM3 at a much higher concentration (1,000 nM) does not stimulate receptor internalization in HEK-sst2 cells. ^nat^Cu-CB-TE2A-LM3 was able to inhibit receptor internalization induced by [Tyr^3^]octreotide. Cellular uptake studies showed that ^64^Cu-CB-TE2A-LM3 bound to the cell surface of HEK-sst2 cells with 30% of the incubation dose at 30 min and ~40% ID at 2-4 h. Internalization of ^64^Cu-CB-TE2A-LM3 was ~13% and was inhibited to 1% incubation dose with excess unlabeled ligand. After 4 h in fresh medium, 70% of radioactivity remained on the cell surface with 15% was internalized and 15% was found in the medium.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CB-TE2A-LM3+and+rodentia)]

Fani et al. (10) performed ex vivo biodistribution studies with 5.55 MBq (0.15 mCi) ^64^Cu-CB-TE2A-LM3 in nude mice (n = 3-7/group) bearing xenografts of HEK-sst2 tumor cells at 1, 4, and 24 h after injection. The accumulation of radioactivity in the SSTR2 tumor was 19.26 ± 3.75% injected dose per gram (% ID/g) at 1 h, 26.87% ID/g at 4 h, and 21.55% ID/g at 24 h after injection. The pancreas had the highest accumulation (43.89% ID/g) at 1 h after injection, followed by the stomach (27.92% ID/g), kidney (19.78% ID/g), lung (8.27% ID/g), liver (5.66% ID/g), and adrenal (6.16% ID/g). Accumulation of radioactivity in the other tissues was low. The concentration in the blood was 0.19% ID/g at 4 h after injection, with tumor/blood ratios of 24, 141, and 127 at 1, 4, and 24 h, respectively. Co-injection with 2,000-fold excess DOTA-LM3 reduced the accumulation of radioactivity by 85% in the tumor, 97% in the stomach, 98% in the pancreas, 99% in the adrenal, and 80% in the lung at 4 h after injection. Little or no inhibition was observed in the other tissues. In comparison, accumulation of ^64^Cu-CB-TE2A-LM3 in the kidney was 1-, 3-, and 8- fold higher than that of ^64^Cu-NODAGA-LM3 at 1, 4, and 24 h, respectively. The tumor/tissue ratios (blood, kidney, liver and muscle) were significantly lower for ^64^Cu-CB-TE2A-LM3 than ^64^Cu-NODAGA-LM3 (P < 0.01). Whole-body PET imaging visualized the SSTR2 tumor at 4 and 24 h after injection of 6 MBq (0.16 mCi) ^64^Cu-CB-TE2A-LM3.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CB-TE2A-LM3+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CB-TE2A-LM3+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CB-TE2A-LM3+and+human)]

No publication is currently available.

## References

1 Weckbecker G., Lewis I., Albert R., Schmid H.A., Hoyer D., Bruns C. (2003). Opportunities in somatostatin research: biological, chemical and therapeutic aspects. Nat Rev Drug Discov.
2 Patel Y.C., Wheatley T. (1983). In vivo and in vitro plasma disappearance and metabolism of somatostatin-28 and somatostatin-14 in the rat. Endocrinology.
3 Corleto V.D., Nasoni S., Panzuto F., Cassetta S., Delle Fave G. (2004). Somatostatin receptor subtypes: basic pharmacology and tissue distribution. Dig Liver Dis.
4 Moller L.N., Stidsen C.E., Hartmann B., Holst J.J. (2003). Somatostatin receptors. Biochim Biophys Acta.
5 Barnett P. (2003). Somatostatin and somatostatin receptor physiology. Endocrine.
6 Krenning E.P., Kwekkeboom D.J., Bakker W.H., Breeman W.A., Kooij P.P., Oei H.Y., van Hagen M., Postema P.T., de Jong M., Reubi J.C., et al. (1993). Somatostatin receptor scintigraphy with [111In-DTPA-D-Phe1]- and [123I-Tyr3]-octreotide: the Rotterdam experience with more than 1000 patients. Eur J Nucl Med.
7 Kwekkeboom D.J., Mueller-Brand J., Paganelli G., Anthony L.B., Pauwels S., Kvols L.K. (2005). M. O'Dorisio T, R. Valkema, L. Bodei, M. Chinol, H.R. Maecke, and E.P. Krenning, Overview of results of peptide receptor radionuclide therapy with 3 radiolabeled somatostatin analogs. J Nucl Med.
8 Storch D., Behe M., Walter M.A., Chen J., Powell P., Mikolajczak R., Macke H.R. (2005). Evaluation of [99mTc/EDDA/HYNIC0]octreotide derivatives compared with [111In-DOTA0,Tyr3, Thr8]octreotide and [111In-DTPA0]octreotide: does tumor or pancreas uptake correlate with the rate of internalization?. J Nucl Med.
9 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
10 Fani M., Del Pozzo L., Abiraj K., Mansi R., Tamma M.L., Cescato R., Waser B., Weber W.A., Reubi J.C., Maecke H.R. (2011). PET of somatostatin receptor-positive tumors using 64Cu- and 68Ga-somatostatin antagonists: the chelate makes the difference. J Nucl Med.